# 6-O-(2-[^18^F]Fluoroethyl)-6-O-desmethyldiprenorphine

Chemical name: | 6-O-(2-[^18^F]Fluoroethyl)-6-O-desmethyldiprenorphine
Abbreviated name: | [^18^F]FDPN
Synonym:
Agent Category: | Compound
Target: | Opioid receptors
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20%28FDPN%20or%20DPN%29)]

Opioids such as morphine are analgesics commonly used in clinical practice. Three opioid receptors (mu, µ; delta, δ; and kappa, κ) that mediate opioid effects have been identified by molecular cloning: δ (enkephalin-preferring), κ (dynorphin-preferring), and µ (ß-endorphin-preferring) (1). Pharmacological studies suggest that each type of opioid receptor consists of subtypes of receptors (2, 3). Their specificity and ubiquitous location are present in both the central and peripheral nervous system. The opioid receptors (G-protein-coupled, resulting in decrease in adenylyl cyclase activity) play an important role in the regulation of analgesia, shock, appetite, thermoregulation, and cardiovascular, mental and endocrine function (2-5). Although the µ opioid receptor is the major receptor to mediate the analgesic effects of opioids, δ and κ receptors are also important in antinociception. Opioids have been found to protect cells from ischemic injury in the heart and brain via the δ receptors. On the other hand, κ antagonists prevent neurodegeneration.

In humans, the κ opioid receptors (κ_1_ and κ_2_ ) are the most abundant brain opioid receptors and are widely distributed in deeper layers of the neocortex (particularly the temporal, parietal, and frontal cortices), striatum, and thalamus, with lower levels in the amygdala, hippocampus, occipital cortex, and cerebellum (6-8). The κ opioid receptors have been implicated in several clinical brain disorders, including drug abuse (9), epilepsy (10), Tourette’s syndrome (11), and Alzheimer’s disease (12).

Diprenorphine is a highly potent and nonselective opioid receptors antagonist with subnanomolar affinity (13). Diprenorphine has been labeled as [6-O-methyl-^11^C]diprenorphine ([^11^C]DPN) (14, 15). [^11^C]DPN is being developed as a positron emission tomography (PET) agent for the non-invasive study of opioid receptors in the brain. However, [^11^C]DPN PET studies are complicated by the 20.4 min short half-life (t_1/2_) of ^11^C. 6-O-(2-[^18^F]Fluoroethyl)-6-O-desmethyldiprenorphine ([^18^F]FDPN) has been synthesized as a ^18^F (t_1/2_ = 110 min) labeled analog of DPN to improve signal intensity, accuracy, and sensitivity of PET studies of opioid receptors in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20%28FDPN%20or%20DPN%29%20and%20synthesis)]

Wester et al. (16) reported synthesis of [^18^F]FDPN by a 3-step reaction, which consisted of ^18^F-fluorination of ethylene glycol-1,2-ditosylate, ^18^F-fluoroethylation of [3-O-trityl-6-O-desmethyl]diprenorphine, and final acidic deprotection of the product. An average radiochemical yield was 22 ± 7% with a total synthesis time of 100 min. An average specific activity was 37 GBq/μmol (1 Ci/μmol at end of synthesis) with a radiochemical purity of >98%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20%28FDPN%20or%20DPN%29%20and%20in%20vitro)]

Chang et al. (17) reported that [^3^H]DPN had a K_d_ of 0.23 nM and a B_max_ of 530 fmol/mg protein in vitro binding assays using rat brain membranes. DPN had K_i_ values of 0.20, 0.18, and 0.47 nM for the µ, δ, and κ opioid receptors, respectively. Therefore, DPN binds to all three subtypes of opioid receptors equally with good affinity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20%28FDPN%20or%20DPN%29%20and%20rodentia)]

Biodistribution studies in female mice injected with 185 MBq (5 mCi) [^18^F]FDPN were performed by Wester et al. (16) showing high accumulation of radioactivity in the brain (4.36 ± 0.49% injected dose (ID) at 5 min post injection) as compared with [^11^C]DPN (7.5 ± 0.89%ID/g). The bulk of accumulation was in the lungs, liver, intestine, and kidneys at 5 min. Clearance of radioactivity occurred at 240 min for all tissues except the bone and intestine, which showed an increase from 0.82%ID/g at 60 min to 1.51%ID/g at 240 min and from 10.3%ID/g at 5 min to 36.85%ID/g at 240 min, respectively. Hence, there is a small trapping of free ^18^F-fluoride in the bone and most of the [^18^F]FDPN is hepatobiliary excreted. The fraction of unchanged [^18^F]FDPN in the brain determined by HPLC was >80% at 30 min after injection. The fraction of unchanged [^18^F]FDPN in plasma samples determined by HPLC was 5% at 30 min after injection with one major hydrophilic metabolite. Ex vivo autoradiographic studies of rat brain at 60 min after injection of 0.0185 MBq (0.5 μCi) [^18^F]FDPN revealed radioactivity in the cerebral cortex, cerebellum, striatum, and thalamus. Pretreatment with 1 mg/kg naloxone blocked the radioactivity to the same level as the cerebellum.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20%28FDPN%20or%20DPN%29%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20%28FDPN%20or%20DPN%29%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20and%20%28FDPN%20or%20DPN%29%20and%20human)]

Wester et al. (16) studied one adult male volunteer with [^18^F]FDPN PET imaging over a period of 90 min. The clearance of the tracer from plasma to tissue from spectral analyses was calculated from the impulse response function at 60 min (IRF_60_, highly correlated with distribution volume) using the arterial input function. High levels of [^18^F]FDPN radioactivity were found in the striatum (IRF_60_ = 0.16101 ± 0.03251), thalamus (IRF_60_ = 0.16839 ± 0.04668), and medial prefrontal cortex (IRF_60_ = 0.16563 ± 0.14703). Low levels were found in the occipital cortex (IRF_60_ = 0.03056 ± 0.01123). The [^18^F]FDPN binding pattern was similar to that of a control group of nine healthy volunteers after injection of [^11^C]DPN. The fraction of unchanged [^18^F]FDPN in plasma samples determined by HPLC was 50% at 15 min after injection.

Spilker et al. (18) evaluated [^18^F]FDPN kinetics in the human brain with compartmental and non-compartmental modeling approaches. The results indicate that a two-tissue compartmental model best characterizes the data obtained following a bolus injection of [^18^F]FDPN (120-min scanning protocol). Estimates of distribution volume (DV) were robust, being highly correlated for the one-tissue compartmental model as well as the Logan model and the basis function method. The binding potential (BP) values showed more variability between methods. BP values were also found to correlate with DV values. Furthermore, the DV estimates were also stable under a shortened protocol of 60 min, showing a significant correlation with the full protocol. However, Boecker et al. (19) concluded from their studies that [^18^F]FDPN PET should be sampled not to be shorter than 90 min.

## References

1 Minami M., Satoh M. (1995). Molecular biology of the opioid receptors: structures, functions and distributions. Neurosci Res.
2 Waldhoer M., Bartlett S.E., Whistler J.L. (2004). Opioid receptors. Annu Rev Biochem.
3 Satoh M., Minami M. (1995). Molecular pharmacology of the opioid receptors. Pharmacol Ther.
4 Molina P.E. (2006). Opioids and opiates: analgesia with cardiovascular, haemodynamic and immune implications in critical illness. J Intern Med.
5 Barry U., Zuo Z. (2005). Opioids: old drugs for potential new applications. Curr Pharm Des.
6 Peckys D., Landwehrmeyer G.B. (1999). Expression of mu, kappa, and delta opioid receptor messenger RNA in the human CNS: a 33P in situ hybridization study. Neuroscience.
7 Hiller J.M., Fan L.Q. (1996). Laminar distribution of the multiple opioid receptors in the human cerebral cortex. Neurochem Res.
8 Simonin F., Gaveriaux-Ruff C., Befort K., Matthes H., Lannes B., Micheletti G., Mattei M.G., Charron G., Bloch B., Kieffer B. (1995). kappa-Opioid receptor in humans: cDNA and genomic cloning, chromosomal assignment, functional expression, pharmacology, and expression pattern in the central nervous system. Proc Natl Acad Sci U S A.
9 Mello N.K., Negus S.S. (2000). Interactions between kappa opioid agonists and cocaine. Preclinical studies. Ann N Y Acad Sci.
10 de Lanerolle N.C., Williamson A., Meredith C., Kim J.H., Tabuteau H., Spencer D.D., Brines M.L. (1997). Dynorphin and the kappa 1 ligand [3H]U69,593 binding in the human epileptogenic hippocampus. Epilepsy Res.
11 Chappell P.B., Leckman J.F., Scahill L.D., Hardin M.T., Anderson G., Cohen D.J. (1993). Neuroendocrine and behavioral effects of the selective kappa agonist spiradoline in Tourette's syndrome: a pilot study. Psychiatry Res.
12 Mathieu-Kia A.M., Fan L.Q., Kreek M.J., Simon E.J., Hiller J.M. (2001). Mu-, delta- and kappa-opioid receptor populations are differentially altered in distinct areas of postmortem brains of Alzheimer's disease patients. Brain Res.
13 Pfeiffer A., Pasi A., Mehraein P., Herz A. (1982). Opiate receptor binding sites in human brain. Brain Res.
14 Lever J.R., Dannals R.F., Wilson A.A., Ravert H.T., Wagner H.N. (1987). Synthesis of carbon-11 labeled diprenorphine: a radioligand for positron emission tomographic studies of opiate receptors. Tetrahedron Letters.
15 Luthra S.K., Brady F., Turton D.R., Brown D.J., Dowsett K., Waters S.L., Jones A.K., Mathews R.W., Crowder J.C. (1994). Automated radiosyntheses of [6-O-methyl-11C]diprenorphine and [6-O-methyl-11C]buprenorphine from 3-O-trityl protected precursors. Appl Radiat Isot.
16 Wester H.J., Willoch F., Tolle T.R., Munz F., Herz M., Oye I., Schadrack J., Schwaiger M., Bartenstein P. (2000). 6-O-(2-[18F]fluoroethyl)-6-O-desmethyldiprenorphine ([18F]DPN): synthesis, biologic evaluation, and comparison with [11C]DPN in humans. J Nucl Med.
17 Chang K.J., Cooper B.R., Hazum E., Cuatrecasas P. (1979). Multiple opiate receptors: different regional distribution in the brain and differential binding of opiates and opioid peptides. Mol Pharmacol.
18 Spilker M.E., Sprenger T., Valet M., Henriksen G., Wagner K., Wester H.J., Toelle T.R., Boecker H. (2004). Quantification of [18F]diprenorphine kinetics in the human brain with compartmental and non-compartmental modeling approaches. Neuroimage.
19 Boecker H., Sprenger T., Henriksen G., Toelle T.R., Spilker M.E. (2005). Optimal duration of PET studies with 18F-fluoroethyl-diprenorphine. J Nucl Med.